# [^99m^Tc(N)(NS-Cys-Gly-CCK-8)(PNP3)]^+^

Chemical name: | [^99m^Tc(N)(NS-Cys-Gly-CCK-8)(PNP3)]^+^
Abbreviated name: | ^99m^Tc(N)(PNP3)-CCK-8
Synonym: | ^99m^Tc-CCK-8
Agent Category: | Peptide
Target: | Gastrin/cholecystokinin-2 (CCK-2, CCK-B) receptor
Target Category: | Receptor binding
Method of detection: | Single-photon emission computed tomography (SPECT), planar gamma imaging
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | ^99m^Tc(N)(PNP3)-CCK-8

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%5BTc%28N%29%28PNP%29%5D2+)]

[^99m^Tc-(N)(NS-Cys-Gly-CCK-8)(PNP3)]^+^ (^99m^Tc(N)(PNP3)-CCK-8) is a radiolabeled peptide developed for single-photon emission computed tomography (SPECT) imaging of tumors that express the gastrin/cholecystokinin-2 (CCK-2) receptor (1). ^99m^Tc is a gamma emitter with a physical half-life (t_½_) of 6.01 h.

The gastrointestinal peptides gastrin and CCK have various regulatory functions in the brain and gastrointestinal tract (2). Gastrin and CCK have the same COOH-terminal pentapeptide amide sequence which is the biologically active site (3). Human gastrin is a peptide composed of 34-amino acids and also exists in several C-terminal truncated forms (4). These C-terminal truncated forms include minigastrin, which is a 13-residue peptide with the sequence of LEEEEEAYGWMDF-NH_2_. CCKs exist in a variety of biologically active molecular forms that are derived from a precursor molecule comprising 115 amino acids (5). These forms range from 4 to 58 amino acids in length and include sulphated and unsulphated CCK-8 which has the structure DYMGWMDF-NH_2_. These forms bind to and act through transmembrane G-protein−coupled receptors (6). Two different CCK receptor subtypes have been identified in normal tissues. CCK-1 (CCK-A, alimentary) receptors have low affinity for gastrin, and CCK-2 (CCK-B, brain) receptors have high affinity for gastrin (5). They also differ in terms of molecular structure, distribution, and affinity for CCK. These receptors have also been found to be expressed or overexpressed on a multitude of tumor types (6). CCK-2 receptors have been found most frequently in medullary thyroid carcinoma, small cell lung cancers, astrocytomas and stromal ovarian cancers (2). CCK-1 receptors have been identified in gastroenteropancreatic tumors, meningiomas and neuroblastoma.

Reubi et al. (7) designed a series of radiolabeled CCK-8 peptides that showed high specificity for potential in vivo imaging of CCK-2 receptor-expressing tumors. de Jong et al (8) developed a ^111^In-labeled nonsulfated CCK-8 analog using DOTA as a bifunctional chelating agent. The radioligand showed high specific internalization rates in the receptor-positive AR42J rat pancreatic tumor cells. von Guggenberg et al (9) reported the synthesis of ^99m^Tc-HYNIC-minigastrin complexes and showed high tumor uptake in nude mice bearing AR42J tumors. Nock et al. (10) prepared 99mTc-labeled minigastrin analogs and found that they displayed high specific localization in nude mice bearing AR42J tumors. Mather et al. (4) synthesized a library of different peptide sequences based on the C-terminal sequences of CCK-8 or minigastrin. Tc mixed-ligand complexes that display characteristic substitution-inert metal fragments [Tc(CO_3_)]^+^ and [Tc(N)(PNP)]^2+^can be used as platforms in the design of potential ^99m^Tc radiopharmaceuticals (11-14). The [Tc(N)(PNP)]^2+^ technology can produce well-defined complexes with very high yields (>90%) depending on the co-ligand (15). Agostini et al (1). applied this technology to the labeling of a nonsulfated CCK-8 peptide analog. PNP3 (N,N-bis(dimethyoxypropylphosphino- ethyl)methoxyethylamine) was selected as the aminodiphosphine ligand. In vivo evaluation of ^99m^Tc(N)(PNP3)-CCK-8 showed rapid and specific targeting to CCK-2 receptors.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Tc%28N%29%28PNP%29%5D2)]

Agostini et al. (1) described the synthesis of ^99m^Tc(N)(PNP3)-CCK-8. The NS-Cys^24^-Gly^25^-Asp^26^Tyr^27^Met^28^Gly^29^Trp^30^Met^31^Asp^32^Phe^33^NH_2_ (NS-Cys-Gly-CCK-8 peptide was prepared by the standard solid-phase peptide synthesis with the use of an automated peptide synthesizer based on the fluorenylmethoxycarbonyl (Fmoc) strategy. The peptide was combined through the terminal carboxylic group of the cysteine residue to produce a COO-functionalized NH_2_, S-cysteine ligand. A glycine residue was introduced as the spacer group. The peptide identity was confirmed by mass spectra with a M_W_ of 1220. This peptide contained cysteine which could bind the [Tc(N)(PNP)]^2+^ moiety either through the [NH_2_, S−] pair or the {O−,S−] pair of donor atoms to yield the corresponding mixed compound with high specific activity. The PNP3 ligand was obtained commercially. Radiolabeling with ^99m^Tc used the “metal fragment” approach by reacting the bifunctional ligand with the metal fragment to produce the monopositive asymmertrical complex.

Two methods of radiolabeling were tested (1). In the two-step procedure, sodium ^99m^Tc pertechnetate (Na^99m^TcO_4_) was added to a mixture of succinic dehydrate (SDH, nitride nitrogen atom donor), stannous chloride (reducing agent), and ethanol. The mixture was incubated at room temperature for 30 min. This produced a mixture of ^99m^Tc-nitrido precursors that contained the [Tc≡N]^2+^ core. Then the PNP3 ligand and the NS-Cys-Gly-CCK-8 peptide were added simultaneously to the mixture (pH 7) and heated at 80ºC for 60 min to produce the final ^99m^Tc(N)(PNP3)-CCK-8. The radiochemical yield (RCY) of this approach was 90.0%. In the one-step (one-pot) procedure, Na^99m^TcO_4_ was added to a mixture of succinic dehydrate, stannous chloride, ethanol, the peptide in phosphate buffer (pH 7.4), and PNP3. The RCY of this procedure was 90.9%. The final monocationic complexes from both procedures were further purified by high-performance liquid chromatography (HPLC) which yielded a radiochemical purity of >95%. The authors suggested that the similar high yield of the one-pot method demonstrated that the PNP ligand stabilized the [^99m^Tc^V^(N)]^2+^ core and promoted the reactivity of the intermediate [^99m^Tc(N)(PNP)]^2+^ moiety for a rapid coordination of PNP3 to form the metal fragment. Thin−layer chromatography revealed that the final asymmetrical ^99m^Tc(N)(PNP3)-CCK-8 consisted of two isomeric forms in the ratio 60:40 (syn/anti) dependent on the orientation of the COO-substituted cysteine pendant group with respect to the central Tc≡N-terminal core. Resolution of this mixture was not possible by HPLC. No specific activity was reported. In a study of the influence of peptide concentration on RCY, the highest RCY (86.6 ± 1.09% to 91.0 ± 3.4%) appeared to be achieved with an amount of peptide in the range of 50−200 μg (4.1 × 10−^5^ to 1.6 × 10−^4^ mmol). In this concentration range (1.13 × 10−^4^ to 2.81 × 10−^5^ M), no significant change in RCY was found with reaction temperature increased to 100ºC. Both shorter reaction time (15 min) and lower temperature (<50ºC) decreased the RCY.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5BTc%28N%29%28PNP%29%5D2%29%20AND%20in%20vitro)]

The in vitro stability of ^99m^Tc(N)(PNP3)-CCK-8 was evaluated by incubation in saline, human serum, or mouse serum at 37ºC for 24 h (1). At different time points, samples were taken for HPLC analysis. The ^99m^Tc-labeled complex was stable in all conditions within the first 3 h. After 24 h, ~80% and 50% of the peptide remained intact in human serum and mouse serum, respectively. The labeled complex was stable in saline and phosphate buffer (pH 7.4) for 24 h and was highly inert to transchelation challenges with excess cysteine or glutathione. Human epidermoid carcinoma A431 cells that overexpress CCK-2 receptors were used in cell binding studies (16). The compound showed high specific binding at 4ºC with an apparent dissociation constant (K_d_) of 19.0 ± 4.6 nmol/liter and the number of binding sites (B_max_) was 7.7 × 10^5^/cell.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5BTc%28N%29%28PNP%29%5D2%29%20AND%20rodentia)]

Agostini et al. (1) conducted the biodistribution studies in nude mice bearing both the A431 s.c. tumor and receptor-negative tumor in the opposite flank. Each mouse received ~1.85 MBq (50 μCi) ^99m^Tc(N)(PNP3)-CCK-8 and was euthanized at 1 h. The radioactivity appeared to clear rapidly from blood and normal tissues (lungs, spleen and muscle). Rapid radioactivity localization was observed in the tumors with the radioactivity level ~0.8% injected dose/g (% ID/g) at 1 h (extrapolated from Figure 4). This represented a four-fold higher level than that of receptor-negative tumors. There were relatively high radioactivity levels in the liver (~0.9% ID/g) and kidneys (~1.8% ID/g). At 1 h, the highest radioactivity level was found in the intestinal tract (~4.3% ID/g). The authors suggested that the clearance of the unbound radioactivity was through the hepatobiliary system. The high intestinal uptake could be minimized by increasing the hydrophilic properties of the labeled peptide.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5BTc%28N%29%28PNP%29%5D2%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5BTc%28N%29%28PNP%29%5D2%29%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5BTc%28N%29%28PNP%29%5D2%29%20AND%20human)]

No publication is currently available.

## References

1 Agostini S., Bolzati C., Didone E., Cavazza-Ceccato M., Refosco F., Aloj L., Arra C., Aurilio M., Tornesello A.L., Tesauro D., Morelli G. (2007). The [Tc(N)(PNP)](2+) metal fragment labeled cholecystokinin-8 (CCK8) peptide for CCK-2 receptors imaging: in vitro and in vivo studies. J Pept Sci.
2 Reubi J.C., Schaer J.C., Waser B. (1997). Cholecystokinin(CCK)-A and CCK-B/gastrin receptors in human tumors. Cancer Res.
3 Aly A., Shulkes A., Baldwin G.S. (2004). Gastrins, cholecystokinins and gastrointestinal cancer. Biochim Biophys Acta.
4 Mather S.J., McKenzie A.J., Sosabowski J.K., Morris T.M., Ellison D., Watson S.A. (2007). Selection of radiolabeled gastrin analogs for Peptide receptor-targeted radionuclide therapy. J Nucl Med.
5 Wang H., Wong P.T., Spiess J., Zhu Y.Z. (2005). Cholecystokinin-2 (CCK2) receptor-mediated anxiety-like behaviors in rats. Neurosci Biobehav Rev.
6 Behr T.M., Behe M.P. (2002). Cholecystokinin-B/Gastrin receptor-targeting peptides for staging and therapy of medullary thyroid cancer and other cholecystokinin-B receptor-expressing malignancies. Semin Nucl Med.
7 Reubi J.C., Waser B. (1996). Unexpected high incidence of cholecystokinin-B/gastrin receptors in human medullary thyroid carcinomas. Int J Cancer.
8 de Jong M., Bakker W.H., Bernard B.F., Valkema R., Kwekkeboom D.J., Reubi J.C., Srinivasan A., Schmidt M., Krenning E.P. (1999). Preclinical and initial clinical evaluation of 111In-labeled nonsulfated CCK8 analog: a peptide for CCK-B receptor-targeted scintigraphy and radionuclide therapy. J Nucl Med.
9 von Guggenberg E., Behe M., Behr T.M., Saurer M., Seppi T., Decristoforo C. (2004). 99mTc-labeling and in vitro and in vivo evaluation of HYNIC- and (Nalpha-His)acetic acid-modified [D-Glu1]-minigastrin. Bioconjug Chem.
10 Nock B.A., Maina T., Behe M., Nikolopoulou A., Gotthardt M., Schmitt J.S., Behr T.M., Macke H.R. (2005). CCK-2/gastrin receptor-targeted tumor imaging with (99m)Tc-labeled minigastrin analogs. J Nucl Med.
11 Boschi A., Bolzati C., Uccelli L., Duatti A., Benini E., Refosco F., Tisato F., Piffanelli A. (2002). A class of asymmetrical nitrido 99mTc heterocomplexes as heart imaging agents with improved biological properties. Nucl Med Commun.
12 Bolzati C., Mahmood A., Malago E., Uccelli L., Boschi A., Jones A.G., Refosco F., Duatti A., Tisato F. (2003). The [(99m)Tc(N)(PNP)](2+) metal fragment: a technetium-nitrido synthon for use with biologically active molecules. The N-(2-methoxyphenyl)piperazyl-cysteine analogues as examples. Bioconjug Chem.
13 Bolzati C., Boschi A., Uccelli L., Tisato F., Refosco F., Cagnolini A., Duatti A., Prakash S., Bandoli G., Vittadini A. (2002). Chemistry of the strong electrophilic metal fragment [(99)Tc(N)(PXP)](2+) (PXP = diphosphine ligand). A novel tool for the selective labeling of small molecules. J Am Chem Soc.
14 Schibli R., Katti K.V., Higginbotham C., Volkert W.A., Alberto R. (1999). In vitro and in vivo evaluation of bidentate, water-soluble phosphine ligands as anchor groups for the organometallic fac-[99mTc(CO)3]+-core. Nucl Med Biol.
15 Bolzati C., Benini E., Cazzola E., Jung C., Tisato F., Refosco F., Pietzsch H.J., Spies H., Uccelli L., Duatti A. (2004). Synthesis, characterization, and biological evaluation of neutral nitrido technetium(V) mixed ligand complexes containing dithiolates and aminodiphosphines. A novel system for linking technetium to biomolecules. Bioconjug Chem.
16 Aloj L., Caraco C., Panico M., Zannetti A., Del Vecchio S., Tesauro D., De Luca S., Arra C., Pedone C., Morelli G., Salvatore M. (2004). In vitro and in vivo evaluation of 111In-DTPAGlu-G-CCK8 for cholecystokinin-B receptor imaging. J Nucl Med.